# N-(2-(1-(4-(2-Methoxyphenyl)piperazinyl)ethyl))-N-(2-(6-[^18^F]fluoro)-pyridinyl)cyclohexanecarboxamide

Chemical name: | N-(2-(1-(4-(2-Methoxyphenyl)piperazinyl)ethyl))-N-(2-(6-[^18^F]fluoro)-pyridinyl)cyclohexanecarboxamide
Abbreviated name: | [^18^F]6FPWAY
Synonym: | [6-Pyridinyl-^18^F]-WAY-100635
Agent Category: | Compound
Target: | 5-HT_1A_ receptors
Target Category: | Receptor-ligand binding
Method of detection: | Positron emission tomography (PET)
Source of signal/contrast: | ^18^F
Activation: | No
Studies: | - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=6-[18F]fluoro-WAY-100635%20OR%20[18F]6FPWAY%20OR%20[6-Pyridinyl-18F]WAY-100635)]

N-(2-1-(1-(4-(2-Methoxyphenyl)piperazinyl)ethyl)-N-(2-(6-[^18^F]fluoro)-pyridinyl)cyclohexanecarboxamide ([^18^F]6FPWAY) is a radioligand developed for positron emission tomography (PET) imaging of serotonin-1A (5-HT_1A_) receptors in the central nervous system (1, 2). It is a selective 5-HT_1A_ antagonist labeled with ^18^F, a positron emitter with a physical t_½_ of 110 min (3, 4).

The serotonin (5-hydroxytryptamine 5-HT) neurotransmission system consists mainly of neurons in the brainstem, with nerve tracts extending from these neurons to many areas of the brain and spinal cord (5). During firing, the neurons release 5-HT, a neurotransmitter that is involved in the modulation of various important physiologic functions and behavior, such as thermoregulation, cardiovascular function, aggressive and sexual behavior, mood, appetite, and the sleep–wake cycle. The effects of 5-HT are mediated by as many as seven classes of receptor populations (5-HT_1_ to 5-HT_7_), many of which also contain several subtypes. There are five receptor subtypes within the G protein-coupled 5-HT_1_ receptor family with the 5-HT_1A_ subtype located primarily in the limbic forebrain (the hippocampus, entorhinal cortex and septum). 5-HT_1A_ receptors appear to function both as presynaptic (somatodendritic) autoreceptors in the raphe nuclei and as postsynaptic receptors in the terminal fields. This receptor subtype is involved in the modulation of emotion and the function of the hypothalamus, and is implicated in the pathogenesis of anxiety, depression, hallucinogenic behavior, motion sickness, dementia, schizophrenia, and eating disorders. A radioligand that can be used to assess the in vivo densities of 5-HT_1A_ receptors and their changes may facilitate investigation of the relationship of these receptors to various neuropsychiatric diseases and aid in the design of novel drugs for their treatment.

Many psychiatric drugs modulate serotonergic transmission or specifically target the 5-HT_1A_ receptors. Various compounds have been radiolabeled for visualization and quantification of these receptors. WAY 100635 was developed as a highly selective, silent antagonist (possessing no intrinsic agonist activity) of 5HT_1A_ receptors at both presynaptic and postsynaptic sites. WAY 100635 radiolabeled with ^11^C at the carbonyl position is an effective radioligand but it is rapidly cleared and metabolized. The short t_½_ of ^11^C also presents some challenges in clinical application of the radiotracer. A radioligand with slower metabolism and labeled with a longer-lived radioisotope would be a better agent for quantitative PET studies. A number of fluorinated derivatives of WAY 100635 have been developed. Sandell et al. (6) reported the synthesis of 6FPWAY and that the presence of a halogen in the pyridine ring appeared to retard its metabolism in primates. 6FPWAY was very different from another WAY analog synthesized by Lang et al. (7) which contained a fluorine in the para position of the benzamide moiety and was abbreviated FPWAY. Recently, Jagoda et al. (8) published a full description of FPWAY, which had previously been referred to as 1,3 pyrimidine WAY.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%286-[18F]Fluoro-WAY-100635%20OR%20[18F]6FPWAY%20OR%20[Pyridinyl-6-18F]WAY%201006350%20AND%20synthesis)]

The nonradioactive reference compound, 6FPWAY, was synthesized by Marchais et al. (9) by a synthesis pathway using 2-amino-6-pyridine as the precursor. In this method, the nucleophilic substitution was performed directly by heating 2,6-difluoropyridine in tetrahydrofuran with an amine nucleophile. The intermediate product was then acylated with cyclohexanecarbonyl chloride to 6FPWAY with a yield of 10%. The precursor, N-(2-1-(1-(4-(2-methoxyphenyl)piperazinyl)ethyl)-N-(2-(6-bromo)-pyridinyl)cyclohexanecarboxamide (6BPWAY) was prepared by oxidizing 2,6-dibromopyridine with hydrogen peroxide. This was then reacted with an amine nucleophile, followed by reduction with iron in acetic acid. Reaction of the product with cyclohexanecarbonyl chloride in dichloromethane gave 6BPWAY with 75% yield.

Karramkam et al. (4) reported the radiosynthesis of [^18^F]6FPWAY. No-carrier-added aqueous [^18^F]fluoride was produced by an [^18^O(p,n)^18^F] nuclear reaction initiated by irradiation of 2 ml of 95% enriched [^18^O]water with a 17 MeV proton beam. 6BPWAY was prepared as the precursor as described by Marchais et al. (9). Introduction of ^18^F was performed in dimethyl sulfoxide with the activated K[^18^F]F-K_222_ complex by conventional heating at 145 ºC for 10 min.

Alternatively, the nitro derivative of WAY 100635 (6NPWAY) could be prepared as the precursor and reacted with [^18^F] fluoride by microwave heating at 100 W for 1 min. With 6-bromopyridine derivative used as the precursor, after Sep-Pak separation, the product that was purified by high performance liquid chromatography (HPLC) was pure [^18^F]6FPWAY. The reported yield was15-25% based on the starting [^18^F]fluoride activity. The synthesis time was 50-70 min, with 0.55-0.92 GBq (15-25 mCi) of [^18^F]6FPWAY obtained from 3.7 GBq (100 mCi) of [^18^F]fluoride. The specific activity was 37-72 GBq (1-2 Ci)/µmol at the end of synthesis. The chemical purity was >95%, and the radiochemical purity was >99%. The radiotracer was radiochemically stable for at least 120 min based on HPLC analysis.

McCarron et al. (2) reacted 6BPWAY with dry [^18^F]fluoride ion at 100 ºC for 20 min and reported a 2% radiochemical decay-corrected yield. The radiochemical purity was >99%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%286-[18F]Fluoro-WAY-100635%20OR%20[18F]6FPWAY%20OR%20[Pyridinyl-6-18F]WAY%201006350%29%20AND%20in%20vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%286-[18F]Fluoro-WAY-100635%20OR%20[18F]6FPWAY%20OR%20[Pyridinyl-6-18F]WAY%201006350%29%20AND%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%286-[18F]Fluoro-WAY-100635%20OR%20[18F]6FPWAY%20OR%20[Pyridinyl-6-18F]WAY%201006350%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%286-[18F]Fluoro-WAY-100635%20OR%20[18F]6FPWAY%20OR%20[Pyridinyl-6-18F]WAY%201006350%29%20AND%20%28primate%20NOT%20human%29)]

McCarron et al. (2) studied the in vivo behavior of [^18^F]6FPWAY with PET imaging in a male cynomolgus monkey. In the first (distribution) study a 28 MBq (0.78 mCi) i.v. dose of [^18^F]6FPWAY (>99% radiochemical purity) was injected, and in the second (blocking) study, a 29 MBq (0.784 mCi) i.v. dose was injected into the same monkey 10 min after i.v. injection of WAY 100635 (0.5 mg/kg). In the distribution study, the radioactivity reached the brain and peaked at 4.33% of injected dose around 7.5 min after injection. Localization of radioactivity in the brain was rapid and was followed by a slower clearance. Radioactivity was localized in regions known to contain high densities of 5-HT_1A_ receptors (e.g., the insula, temporal, and frontal cortex). The tissue/cerebellum radioactivity ratio was highest (~2) in the insula after 30 min. The second highest ratio was in the cingulated gyrus. When WAY 100635 was administered in the blocking study, there was notably much less radioactivity in brain 5-HT_1A_ receptor-rich regions. The tissue/cerebellum ratios were also lower for these regions. HPLC analysis of blood samples obtained from the monkey showed two main peaks of radioactive metabolites. One metabolite was possibly [^18^F]descyclohexylcarbonyl-6FPWAY (comigrated with the metabolite in HPLC), and it represented about 19% of radioactivity in the plasma at 55 min. This indicated that amide scission was likely the major route of metabolism. [^18^F]Descyclohexylcarbonyl-6FPWAY was possibly able to cross the blood-brain barrier (BBB). The lack of radioactivity on the skull might indicate that rapid defluorination did not occur. The researchers suggested that the position 6 of the pyridinyl ring in the [^18^F]6FPWAY was a metabolically resistant site for ^18^F labeling. The first WAY 100635 analog was radiolabeled with ^11^C at the methoxyphenyl position. On hydrolysis of the amide in humans, the radiolabeled metabolite crossed the BBB (10).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%286-[18F]Fluoro-WAY-100635%20OR%20[18F]6FPWAY%20OR%20[Pyridinyl-6-18F]WAY%201006350%29%20AND%20human)]

No publication is currently available.

## NIH Support

NIH Intramural Support.

## References

1 Passchier J., van Waarde A. (2001). Visualisation of serotonin-1A (5-HT1A) receptors in the central nervous system. Eur J Nucl Med.
2 McCarron J.A., Pike V.W., Halldin C., Sandell J., Sovago J., Gulyas B., Cselenyi Z., Wikstrom H.V., Marchais-Oberwinkler S., Nowicki B., Dolle F., Farde L. (2004). The pyridinyl-6 position of WAY-100635 as a site for radiofluorination--effect on 5-HT1A receptor radioligand behavior in vivo. Mol Imaging Biol.
3 Bantick R.A., Rabiner E.A., Hirani E., de Vries M.H., Hume S.P., Grasby P.M. (2004). Occupancy of agonist drugs at the 5-HT1A receptor. Neuropsychopharmacology.
4 Karramkam M., Hinnen F., Berrehouma M., Hlavacek C., Vaufrey F., Halldin C., McCarron J.A., Pike V.W., Dolle F. (2003). Synthesis of a [6-pyridinyl-18F]-labelled fluoro derivative of WAY-100635 as a candidate radioligand for brain 5-HT1A receptor imaging with PET. Bioorg Med Chem.
5. Sunderland, P.M., Structure and function of the nervous system, in Pathophysiology: The biologic basis for disease in adults and children, K.L. McCance, and S.H. Huether, Editor. 1994, Mosby-Year Book, Inc.: St. Louis, MO. p. 397-436.
6 Sandell J., Halldin C., Pike V.W., Chou Y.H., Varnas K., Hall H., Marchais S., Nowicki B., Wikstrom H.V., Swahn C.G., Farde L. (2001). New halogenated [11C]WAY analogues, [11C]6FPWAY and [11C]6BPWAY--radiosynthesis and assessment as radioligands for the study of brain 5-HT1A receptors in living monkey. Nucl Med Biol.
7 Lang L., Jagoda E., Schmall B., Vuong B.K., Adams H.R., Nelson D.L., Carson R.E., Eckelman W.C. (1999). Development of fluorine-18-labeled 5-HT1A antagonists. J Med Chem.
8 Jagoda E.M., Lang L., Tokugawa J., Simmons A., Ma Y., Contoreggi C., Kiesewetter D., Eckelman W.C. (2006). Development of 5-HT(1A) receptor radioligands to determine receptor density and changes in endogenous 5-HT. Synapse.
9 Marchais S., Nowicki B., Wikstrom H., Brennum L.T., Halldin C., Pike V.W. (2001). Short and efficient syntheses of analogues of WAY-100635: new and potent 5-HT1A receptor antagonists. Bioorg Med Chem.
10 Osman S., Lundkvist C., Pike V.W., Halldin C., McCarron J.A., Swahn C.G., Farde L., Ginovart N., Luthra S.K., Gunn R.N., Bench C.J., Sargent P.A., Grasby P.M. (1998). Characterisation of the appearance of radioactive metabolites in monkey and human plasma from the 5-HT1A receptor radioligand, [carbonyl-11C]WAY-100635--explanation of high signal contrast in PET and an aid to biomathematical modelling. Nucl Med Biol.